# ^99m^Tc-Anti-ED-B fibronectin single-chain antibody fragment L19-Hi20

Chemical name: | ^99m^Tc-Anti-ED-B fibronectin single-chain antibody fragment L19-Hi20
Abbreviated name: | ^99m^Tc-L19-Hi20
Synonym: | ^99m^Tc-scFv L19-Hi20, ^99m^Tc-anti-ED-B FN ScFv Ab
Agent Category: | Single-chain Antibody fragment (scFv)
Target: | ED-B Fibronectin (ED-B FN)
Target Category: | Antibody-antigen binding
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov). Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=5725426), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=31406) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=407105) for more information about ED-B fibronectin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2899mTc-L19-Hi20%29%20OR%20%28Radiolabeled%20anti-fibronectin%20antibody%29)]

^99m^Tc-Anti-ED-B fibronectin single-chain antibody fragment L19-Hi20 (^99m^Tc-L19-Hi20) is a radiolabeled molecular imaging agent developed for single-photon emission computed tomography (SPECT) imaging of tumor angiogenesis and guidance for antiangiogenic treatment (1). ^99m^Tc is a gamma emitter with a half-life (t_½_) of 6.01 h.

Angiogenesis is a process of development and growth of new blood vessels from pre-existing vessels (2). Tumor growth depends on the formation of new blood vessels from this process. Normal angiogenesis is orderly and highly regulated, whereas tumor angiogenesis is chaotic and irregular. Abnormal angiogenesis is important in the carcinogenesis, growth, and progression of solid and hematologic tumors in humans (3). Fibronectins (FNs) are a family of universal cell-adhesion molecules that are widely distributed (1). FN is a polymorphic glycoprotein of ~2500 amino acids and has a high molecular mass of 250–280 kDa. FN occurs in soluble form in plasma and other body fluids and in insoluble form in the extracellular matrices (4, 5). Both forms are dimers composed of a series of repeating units of three types and joined by two disulfide bonds at the C-terminus of the molecule. FN polymorphism arises from alternative splicing patterns of the pre-mRNA or post-translational modifications of FN itself (5). The splice variant ED-B FN, which is highly expressed during angiogenesis in both neoplastic and normal tissues (6), is an oncofetal antigen expressed at different levels in the stroma associated with the neovasculature of solid tumors. High levels of ED-B expression have been found in primary and metastatic tumors in breast, colorectal, and non-small cell lung cancers (1, 7-9).

Molecular imaging of angiogenesis offers serial non-invasive evaluation of both location and growth dynamics of tumors (10). SPECT or positron emission tomography imaging with an appropriate radiolabeled tracer targeted to angiogenic pathways may allow the evaluation of specific aspects of tumor vascular biology (9). A molecular probe that targets ED-B FN can be both an early tumor marker and a tool to monitor the success of antiangiogenic cancer therapy. The single-chain antibody fragment (scFv) L19, which has a high affinity for ED-B FN, was developed by Pini et al. (11). Radioiodinated L19 showed specific accumulation around tumor neovasculature and tumor stroma with high ED-B expression (12, 13). In an effort to prepare a stable ^99m^Tc-labeled L19, Berndorff et al. (1) chemically modified L19 with a bifunctional MAG2-type chelator (L19-Hi20). Two other L19 derivatives, AP39 and L19-His, were also prepared for radiolabeling. These ^99m^Tc-labeled L19 derivatives appeared to have favorable biodistribution and imaging properties in mice bearing murine embryonal teratocarcinomas (F9). However, the study did not provide data to confirm that the binding was a result of angiogenesis.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc-L19-Hi20%29%20OR%20%28Radiolabeled%20anti-fibronectin%20antibody%29%29%20AND%20synthesis)]

Pini et al. (11) constructed and used a large synthetic phage display human antibody library (>3 × 10^8^ clones) to produce L19 with a very high affinity (dissociation constant (K_d_) = 54 pM) for the ED-B domain of FN. L19 was cloned in scFv configuration in the novel phagemid vector pDN332. L19 was then chemically modified by the chelator 2-tertbutyldisulfanyl-N-({[(4-isothiocyanatobutylcarbamoyl)methyl]carbamoyl}-methyl)acetamide (Hi20) (1). Hi20 was conjugated to ε-NH_2_ groups of L19. Briefly, L19 was dissolved in phosphate-buffered saline (PBS, pH 7.4) and dialyzed twice with sodium borate buffer (pH 8.5) by a 10-kDa molecular weight cut-off membrane. Hi20 was then dissolved in N,N-dimethylformamide and added to dialyzed L19. The mixture was incubated for 3 h at 37ºC and then allowed to cool to room temperature. L19-Hi20 was then dialyzed. Before radiolabeling, L19-Hi20 was reduced by the addition of tris-(2-carboxyethyl)phosphine-hydrochloride in sodium phosphate buffer (pH 7.4) and incubated at 37ºC for 1 h. The reduced form of L19-Hi20 was purified via gel chromatography. The purified reduced L19-Hi20 (110 μg) was mixed with sodium tartrate dehydrate, phosphate buffer (pH 10.5), 70 MBq (1.89 mCi) ^99m^Tc pertechnetate, and stannous chloride. The mixture was incubated for 30 min at 37ºC. ^99m^Tc- L19-Hi20 was purified by NAP-5 affinity chromatography. The radiochemical yield was 54% with a radiochemical purity >91%. Size-exclusion high-performance liquid chromatography analysis showed that ^99m^Tc- L19-His was a monomer/dimer mixture. The specific activity was 21 MBq/nmol (dimer; 0.57 mCi/nmol). The yield was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc-L19-Hi20%29%20OR%20%28Radiolabeled%20anti-fibronectin%20antibody%29%29%20AND%20in%20vitro)]

Berndorff et al. (1) determined the in vitro immunoreactivity of ^99m^Tc-L19-Hi20 by using affinity chromatography with ED-B FN-conjugated Sepharose. ^99m^Tc-L19-Hi20 showed an immunoreactivity of 82%.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc-L19-Hi20%29%20OR%20%28Radiolabeled%20anti-fibronectin%20antibody%29%29%20AND%20rodentia)]

Biodistribution studies (n = 3) of ^99m^Tc-L19-Hi20 were performed in nude mice bearing murine F9 tumors (1). F9 tumors were previously reported to express high levels of ED-B FN (13). ^99m^Tc-L19-Hi20 showed rapid blood clearance and radioactivity localization in the tumor. The radioactivity levels of ^99m^Tc-L19-Hi20 (percentage of injected dose per g (% ID/g)) in the tumors were 3.5 ± 0.6 (0.25 h), 6.8 ± 1.9 (1 h), 7.7 ± 2.1 (3 h), 7.6 ± 0.6 (5 h), and 4.0 ± 2.6 (24 h). The tumor/blood ratios were 0.2 ± 0.1 (0.25 h), 0.7 ± 0.2 (1 h), 1.8 ± 0.5 (3 h), 2.7 ± 0.4 (5 h), and 9.4 ± 6.4 (24 h). ^99m^Tc-L19-Hi20 appeared to be excreted primarily by the kidneys radioactivity levels in the kidneys were 33.5 ± 2.4% ID/g and 3.0 ± 0.6% ID/g at 0.25 and 24 h, respectively. Approximately 57.8% ID was excreted via the urine after 24 h. Radioactivity also accumulated in the ED-B FN-expression reproductive organs (ovaries, and uterus). Elevated radioactivity levels were also observed in the spleen, liver, lung, and bone. At 0.25 h, the radioactivity levels (% ID/g) in other major organs were 7.6 ± 4.1 (ovaries), 16.1 ± 1.7 (blood), 9.4 ± 1.4 (lung), 10.5 ± 2.1 (liver), 4.9 ± 0.5 (spleen), 3.5 ± 1.4 (thyroid), 2.1 ± 0.8 (uterus), 4.0 ± 0.4 (bone), and 1.9 ± 0.1 (stomach). By 24 h, these radioactivity levels (% ID/g) decreased to 2.8 ± 0.5 (ovaries), 5.7 ± 2.0 (blood), 1.0 ± 0.2 (bone) 1.7 ± 0.2 (liver), 0.5 ± 0.1 (spleen), 1.6 ± 0.7 (uterus), 0.7 ± 0.1 (thyroid), 1.3 ± 0.5 (lung), 1.0 ± 0.1 (bone), and 0.6 ± 0.1 (stomach). No specific blocking study was performed.

Gamma imaging was performed in mice bearing s.c. F9 tumors (80–100 mm^2^) (1). Each mouse was injected with 4–7 MBq (0.11–0.19 mCi) ^99m^Tc-L19-Hi20. Imaging with ^99m^Tc-L19-Hi20 showed visible tumors at 5 and 24 h. The background was relatively high at 5 h with radioactivity in the liver and kidney. The background radioactivity was cleared after 24 h to produce a low background and clear tumor image.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc-L19-Hi20%29%20OR%20%28Radiolabeled%20anti-fibronectin%20antibody%29%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc-L19-Hi20%29%20OR%20%28Radiolabeled%20anti-fibronectin%20antibody%29%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%2899mTc-L19-Hi20%29%20OR%20%28Radiolabeled%20anti-fibronectin%20antibody%29%29%20AND%20human)]

No publication is currently available.

## References

1 Berndorff D., Borkowski S., Moosmayer D., Viti F., Muller-Tiemann B., Sieger S., Friebe M., Hilger C.S., Zardi L., Neri D., Dinkelborg L.M. (2006). Imaging of tumor angiogenesis using 99mTc-labeled human recombinant anti-ED-B fibronectin antibody fragments. J Nucl Med.
2 Shinkaruk S., Bayle M., Lain G., Deleris G. (2003). Vascular endothelial cell growth factor (VEGF), an emerging target for cancer chemotherapy. Curr Med Chem Anticancer Agents.
3 Ranieri G., Patruno R., Ruggieri E., Montemurro S., Valerio P., Ribatti D. (2006). Vascular endothelial growth factor (VEGF) as a target of bevacizumab in cancer: from the biology to the clinic. Curr Med Chem.
4 Carnemolla B., Balza E., Siri A., Zardi L., Nicotra M.R., Bigotti A., Natali P.G. (1989). A tumor-associated fibronectin isoform generated by alternative splicing of messenger RNA precursors. J Cell Biol.
5 Kosmehl H., Berndt A., Katenkamp D. (1996). Molecular variants of fibronectin and laminin: structure, physiological occurrence and histopathological aspects. Virchows Arch.
6 Castellani P., Viale G., Dorcaratto A., Nicolo G., Kaczmarek J., Querze G., Zardi L. (1994). The fibronectin isoform containing the ED-B oncofetal domain: a marker of angiogenesis. Int J Cancer.
7 Kaczmarek J., Castellani P., Nicolo G., Spina B., Allemanni G., Zardi L. (1994). Distribution of oncofetal fibronectin isoforms in normal, hyperplastic and neoplastic human breast tissues. Int J Cancer.
8 Pujuguet P., Hammann A., Moutet M., Samuel J.L., Martin F., Martin M. (1996). Expression of fibronectin ED-A+ and ED-B+ isoforms by human and experimental colorectal cancer. Contribution of cancer cells and tumor-associated myofibroblasts. Am J Pathol.
9 Santimaria M., Moscatelli G., Viale G.L., Giovannoni L., Neri G., Viti F., Leprini A., Borsi L., Castellani P., Zardi L., Neri D., Riva P. (2003). Immunoscintigraphic detection of the ED-B domain of fibronectin, a marker of angiogenesis, in patients with cancer. Clin Cancer Res.
10 Laking, G.R. and P.M. Price, Positron emission tomographic imaging of angiogenesis and vascular function. Br J Radiol, 2003. 76 Spec No 1: p. S50-9.
11 Pini A., Viti F., Santucci A., Carnemolla B., Zardi L., Neri P., Neri D. (1998). Design and use of a phage display library. Human antibodies with subnanomolar affinity against a marker of angiogenesis eluted from a two-dimensional gel. J Biol Chem.
12 Tarli L., Balza E., Viti F., Borsi L., Castellani P., Berndorff D., Dinkelborg L., Neri D., Zardi L. (1999). A high-affinity human antibody that targets tumoral blood vessels. Blood.
13 Borsi L., Balza E., Bestagno M., Castellani P., Carnemolla B., Biro A., Leprini A., Sepulveda J., Burrone O., Neri D., Zardi L. (2002). Selective targeting of tumoral vasculature: comparison of different formats of an antibody (L19) to the ED-B domain of fibronectin. Int J Cancer.